# (1-Butyl-4-piperidinylmethyl)-8-amino-7-[^123^I]iodo-1,4-benzodioxan-5-carboxylate

Chemical name: | (1-Butyl-4-piperidinylmethyl)-8-amino-7-[^123^I]iodo-1,4-benzodioxan-5-carboxylate
Abbreviated name: | [^123^I]SB207710
Synonym:
Agent category: | Compound
Target: | 5-HT_4_ serotonin receptors
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710)]

Serotonin (5-hydroxytryptamine (5-HT)) has diverse physiological roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It is also a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4).

5-HT_4_ receptors are G-protein–coupled and present in several organs and tissues (5-11). 5-HT_4_ receptors are abundantly present in the hippocampus, hypothalamus, and striatum, and the lowest density is observed in the cerebellum (12). Some thalamic nuclei have intermediate densities. 5-HT_4_ receptors are involved in the mediation of cognition and memory. Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_4_ receptors. (1-Butyl-4-piperidinylmethyl)-8-amino-7-iodo-1,4-benzodioxan-5-carboxylate (SB207710) is a selective, high-affinity 5-HT_4_ receptor antagonist (7, 13). ^123^I-Labeled SB207710 ([^123^I]SB207710) has been evaluated as a single-photon emission tomography (SPECT) radioligand for imaging brain 5-HT_4_ receptors in vivo (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710%20and%20synthesis)]

SB207715 was labeled with sodium [^123^I]iodide according to the chloramine-T method. [^123^I]SB207710 was purified with high-performance liquid chromatography with a radiochemical purity of >99% and radiochemical yields of 60–90% (decay-corrected). The specific activity of [^123^I]SB207710 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710%20and%20in%20vitro)]

SB207710 (0.03–1 nM) antagonized the 5-HT_4_ receptor–mediated relaxations of the carbachol-contracted rat isolated esophagus against 5-HT with a pKB value of 10.9 ± 0.1 (7). Using human postmortem brain sections, the specific binding of [^125^I]SB207710 was highest in regions of the basal ganglia (caudate nucleus, putamen, nucleus accumbens, globus pallidus, and substantia nigra) and the hippocampus, with intermediate density in the neocortex and low density in the cerebellum (15). Cross reactivity with other 5-HT subtypes was not determined.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710%20and%20rodentia)]

Pike et al. (14) reported biodistribution studies of [^125^I]SB207710 in rat brains showing an initial accumulation of ~0.25% injected dose (ID)/g in the striatum, hippocampus, hypothalamus, and cerebellum, followed by a more rapid decrease in radioactivity in the cerebellum. Regional brain distribution displayed peak radioactivity concentrations that followed a rank order (tissue/cerebellum ratio) at 45–75 min after injection: striatum (3.4), hypothalamus (3.1), hippocampus (2.2), amygdale (1.9), thalamus (1.7), frontal cortex (1.2), temporal cortex (1.2), and cerebellum (1.0). Blood and plasma exhibited radioactivity levels of <1% ID/g at 1 min after injection. No blocking studies were presented.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710%20and%20nonhuman%20primate)]

Pike et al. studied SPECT imaging (14) in the brain of a rhesus monkey after intravenous injection of 86 MBq (2.32 mCi) [^123^I]SB207710. The peak accumulation in the whole brain was 2.28% ID at 18.25 min after tracer injection. Various brain regions exhibited rapid accumulation at 8–20 min with gradual decreases thereafter. SPECT images (up to 180 min after injection) displayed radioactivity concentrations that followed a rank order (tissue/cerebellum ratio) at 169 min: striatum (4.0), frontal cortex (3.1), temporal cortex (2.5), and cerebellum (1.0). Pretreatment with SB207710 (0.5 mg/kg) 20 min prior to injection of [^123^I]SB207710 markedly reduced the radioactivity in the regions of interest to homogeneity at 90 min after tracer injection. The striatum/cerebellum, frontal cortex/cerebellum, and temporal cortex/cerebellum ratios at 176 min were 1.1, 1.4, and 1.3, respectively. The peak accumulation in the whole brain was 1.7% ID at 14.5 min after tracer injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SB%20207710%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program, MH44814

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Bach T., Syversveen T., Kvingedal A.M., Krobert K.A., Brattelid T., Kaumann A.J., Levy F.O. (2001). 5HT4(a) and 5-HT4(b) receptors have nearly identical pharmacology and are both expressed in human atrium and ventricle. Naunyn Schmiedebergs Arch Pharmacol.
6 Brattelid T., Kvingedal A.M., Krobert K.A., Andressen K.W., Bach T., Hystad M.E., Kaumann A.J., Levy F.O. (2004). Cloning, pharmacological characterisation and tissue distribution of a novel 5-HT4 receptor splice variant, 5-HT4(i). Naunyn Schmiedebergs Arch Pharmacol.
7 McLean P.G., Coupar I.M. (1995). 5-HT4 receptor antagonist affinities of SB207710, SB205008, and SB203186 in the human colon, rat oesophagus, and guinea-pig ileum peristaltic reflex. Naunyn Schmiedebergs Arch Pharmacol.
8 Sakurai-Yamashita Y., Takada K., Takemura K., Yamashita K., Enjoji A., Kanematsu T., Taniyama K. (1999). Ability of mosapride to bind to 5-HT4 receptor in the human stomach. Jpn J Pharmacol.
9 Sakurai-Yamashita Y., Yamashita K., Kanematsu T., Taniyama K. (1999). Localization of the 5-HT(4) receptor in the human and the guinea pig colon. Eur J Pharmacol.
10 Sakurai-Yamashita Y., Yamashita K., Yoshimura M., Taniyama K. (2000). Differential localization of 5-hydroxytryptamine3 and 5-hydroxytryptamine4 receptors in the human rectum. Life Sci.
11 Yoshida A. (2002). S.Y. Y, M. Kaibara, K. Taniyama, and N. Tanaka, 5-Hydroxytryptamine receptors, especially the 5-HT4 receptor, in guinea pig urinary bladder. Jpn J Pharmacol.
12 Arranz B., Rosel P., San L., Sarro S., Navarro M.A., Marcusson J. (1998). Characterization of the 5-HT4 binding site in human brain. J Neural Transm.
13 Kaumann A.J., Gaster L.M., King F.D., Brown A.M. (1994). Blockade of human atrial 5-HT4 receptors by SB 207710, a selective and high affinity 5-HT4 receptor antagonist. Naunyn Schmiedebergs Arch Pharmacol.
14 Pike V.W., Halldin C., Nobuhara K., Hiltunen J., Mulligan R.S., Swahn C.G., Karlsson P., Olsson H., Hume S.P., Hirani E., Whalley J., Pilowsky L.S., Larsson S., Schnell P.O., Ell P.J., Farde L. (2003). Radioiodinated SB 207710 as a radioligand in vivo: imaging of brain 5-HT4 receptors with SPET. Eur J Nucl Med Mol Imaging.
15 Varnas K., Halldin C., Pike V.W., Hall H. (2003). Distribution of 5-HT4 receptors in the postmortem human brain--an autoradiographic study using [125I]SB 207710. Eur Neuropsychopharmacol.